# VivoTag-S680–conjugated 3-aminomethyl α_v_β_3_ antagonist derivative for fluorescence molecular tomography of tumors

Chemical name: | VivoTag-S680–conjugated 3-aminomethyl α_v_β_3_ antagonist derivative for fluorescence molecular tomography of tumors | [image]
Abbreviated name: | IntegriSense | [image]
Synonym: | | [image]
Agent Category: | Compound | [image]
Target: | Integrins α_v_β_3_/α_v_β_5_ | [image]
Target Category: | Receptor | [image]
Method of detection: | Optical imaging (fluorescence molecular tomography) | [image]
Source of signal / contrast: | VivoTag-S680 | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of IntegriSense. Click on for gene information (http://www.ncbi.nlm.nih.gov/nucleotide/?term=Integrin+Alphavbeta3+and+homo) about integrin α_v_β_3._

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=integrins+and+targeting)]

Integrins are transmembrane glycoproteins with two noncovalently bound α and β subunits. The two subunits mediate cell–cell and cell–extracellular matrix (ECM) interactions, and they act downstream of several primary signaling events that lead to angiogenesis (1-3). Integrins comprise a large family of cell adhesion molecules, and integrin α_v_β_3_ appears to be the most attractive member for angiogenesis-targeted imaging and therapy because of its critical involvement in tumor angiogenesis, development, and metastasis (1, 2). Integrin α_v_β_3_ is minimally expressed in normal blood vessels but is significantly upregulated in newly sprouting vasculature in tumors (4, 5).

A significant effort has been made to generate various imaging agents targeting integrin α_v_β_3_ (6-10). Generally, these agents can be categorized as antibodies, peptides, small-molecule peptidomimetics, and targeted nanoparticles. Vitaxin is the representative of monoclonal antibodies against integrin α_v_β_3_. Vitaxin is a humanized antibody composed of human IgG-1, kappa, and the complement domain regions of the murine antibody LM 609. Regardless of its efficacy in inhibiting angiogenesis, imaging with ^99m^Tc-labeled Vitaxin failed to show the tumor angiogenesis in the clinical settings because of its poor stability and rapid plasma clearance with low doses (11). Interestingly, Gutheil et al. have reported that second-generation Vitaxin-2–conjugated, gadolinium-encapsulated nanoparticles could provide enhanced and detailed imaging of rabbit carcinomas and imaging of angiogenic “hot spots” that are not seen with standard magnetic resonance imaging (12). The major limitations of monoclonal antibodies include large molecular size, low production yield, incomplete tumor penetration, and immunogenicity to host.

Numerous small peptides have been identified to specifically interact with tumor neovasculature, including arginine-glycine-aspartic acid (RGD), asparagine-glycine-arginine, histidine-tryptophan-glycine-phenylalanine, and arginine-arginine-leucine (RRL) (9, 13-15). RGD tripeptide sequence is known as a cell recognition site for adhesive proteins present in the ECM and in blood. Integrin α_v_β_3_ binds ECM proteins through the exposed RGD tripeptide in their ligands. Both linear and cyclic RGD peptide agents have been proven to be useful in imaging tumor neovasculature. In general, linear peptides are broken down rapidly in vivo and occupy a wide range of conformations, resulting in low binding affinity and less specific accumulation within tumors. Short cyclic peptides are superior to linear peptides for their pharmacokinetics due to the fact that they are trapped in the active conformation and are more resistant to proteolysis. The pharmacokinetic behaviors of RGD peptides can be further improved with introduction of sugar moiety, the dimeric format of RGD peptides, or coupling with 1,4,7,10-tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid or polyethylene glycol (13, 16, 17). However, RGD peptides are less selective (binding with 8 of the 24 integrins), and their binding affinities are relatively low (50% inhibition concentration (IC_50_), 20–70 nmol) compared to antibodies. Other peptide sequences such as RRL have also been investigated to generate imaging agents (15, 18). Recently, several classes of peptidomimetic integrin α_v_β_3_ antagonists have been reported (9, 14). These peptidomimetic antagonists consist of a rigid core scaffold bearing basic and acidic groups that mimic the guanidine and carboxylate groups of the RGD sequence. Additionally, ligand array of integrin antagonists on nanoparticles has been proven to be a viable strategy to target vascular surface receptors on endothelial cells. Imaging studies are in progress with these new strategies (7).

Coleman et al. and Wang et al. synthesized a series of 3-substituted tetrahydro-[1,8]naphthyridine–containing α_v_β_3_ antagonists, and the investigators reported that these compounds displayed excellent pharmacokinetics in vivo (19, 20). On the basis of these non-peptide antagonists, Kossodo et al. synthesized a 3-aminomethyl analog, labeled it with fluorescent dye VivoTag-S680, and named the labeled analog IntegriSense (9). IntegriSense had a stronger binding affinity with integrin α_v_β_3_ (IC_50_, 4.1 nmol) and a better selectivity (binding with α_v_β_3_/α_v_β_5_) than RGD peptides. IntegriSense specifically accumulated in the α_v_β_3_/α_v_β_5_-expressing tumors, and the accumulated amount could be quantified in vivo in small animals with fluorescence molecular tomography (FMT). FMT quantifies fluorescence by tomographic reconstruction of a series of fluorescence images excited at different source locations, using a model of photon propagation in a scattering medium (9, 21). By normalizing each fluorescence image to its corresponding excitation image, FMT overcomes the optical heterogeneity of biological tissue, thus resolving the ambiguity about depth, size, and concentration of fluorescence that affects planar imagers. Quantification of known concentrations of fluorochrome with FMT have shown strong linearity between actual and reconstructed FMT dye concentrations and a detection threshold of ~100 fmol (22). FMT has been used for concurrent imaging and quantification of different targets and biological processes (9, 21).

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=integrin+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Articles about integrins in OMIM (http://www.ncbi.nlm.nih.gov/omim/?term=integrins)
- Integrin α_v_β_3_-related clinical trials in ClinicalTrials.gov (http://clinicaltrials.gov/ct2/results?term=Integrin+%CE%B1v%CE%B23)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=non-peptide+%CE%B1v%CE%B23)]

Coleman et al. and Wang et al. described the synthesis of the parent non-peptide α_v_β_3_ antagonists in detail (19, 20). Kossodo et al. first converted the parent antagonist to the 3-cyano derivative on the tetrahydro-1,8-naphthyridine moiety, which was then reduced to the 3-aminomethyl analog (9). This 3-aminomethyl α_v_β_3_ antagonist derivative was conjugated with VivoTag-S680, an amine-reactive near-infrared fluorochrome, to generate the imaging agent IntegriSense (refer to the structure above). The absorption and emission spectra of IntegriSense in phosphate buffered saline were 674/692 nm. The purity and labeling efficiency were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=dual+imaging+and+fluorescence+molecular+tomography+and+integrin+and+protease)]

Kossodo et al. evaluated the affinity and selectivity of IntegriSense for different integrins using human embryonic kidney 293 cells stably expressing human α_v_β_3_, α_IIb_β_3_, α_v_β_5_, or α_5_β_1_ (9). IntegriSense bound to the α_v_β_3_ receptors on the surface of cells, and the binding was blocked by the parent compound. Internalization was observed at 37°C, but not at 4°C. The equilibrium binding constant was 4.2 ± 0.6 nmol, and the dissociation rate constant was 1.08 × 10−^4^ s−^1^ (t_1/2_ = 107 min). Selectivity analysis showed that IntegriSense exhibited stronger affinity for α_v_β_3_ integrin than for α_IIb_β_3_ (9-fold higher) or α_v_β_5_ (8-fold higher), while no specific binding to α_5_β_1_ was detected. Compared to the parent compound, IntegriSense presented a 5-fold loss of affinity to α_v_β_3_ (IC_50_, 4.1 ± 0.3 nmol) and a 25-fold loss of affinity to α_v_β_5_ (IC_50_, 33 nmol). These results indicated that IntegriSense had a high binding affinity for α_v_β_3_ and predominantly bound with its active form. Only binding to the active form of α_v_β_3_ can result in ligand internalization (endocytosis) and accumulation in the cells.

The specificity of IntegriSense to target α_v_β_3_/α_v_β_5_ was further validated with human umbilical vein endothelial cells (HUVEC, used as a surrogate for primary endothelial cells) and human rhabdomyosarcoma A673 tumors cells in vitro. Significant fluorescent signal was observed for both HUVEC and A673 cells, and the fluorescence intensity was reduced in the presence of a blocking dose of parent compound. No fluorescence was detected in cells incubated with free dye alone. Western blot analysis confirmed the expression of the α_v_ subunit both in the A673 cell line and in A673 tumor xenografts ex vivo, supporting the premise that IntegriSense specifically bound to integrin-expressing tumors and endothelial cells in vivo (see below) (9).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=dual+imaging+and+fluorescence+molecular+tomography+and+integrin+and+protease)]

The pharmacokinetics of IntegriSense were first studied in 24 retired female breeder BALB/c mice (9). The concentration dependence of IntegriSense in plasma was fitted into a two-compartment model with a calculated t(1)_1/2_ = 6 min and t(2)_1/2_ = 210 min. The t(1)_1/2_ represented the quick clearing of free IntegriSense from circulation, while the longer t(2)_1/2_ likely corresponded to the clearance of bound IntegriSense. The pharmacodynamics and biodistribution of IntegriSense were then assessed in MDA-MB231, HCT116, A673, and HT29 human tumor xenograft models. MDA-MB231 (breast cancer), HCT116 (colon cancer), and A673 tumors are known to be positive for α_v_β_3_, while HT29 tumors (colon cancer) are negative for α_v_β_3_ but positive for α_v_β_5_.

Biodistribution in A673 tumor-bearing athymic mice 24 h after agent injection showed predominant localization in the tumor, followed by localization in the liver, small intestine, and skin. Confocal microcopy of the A673 tumor sections dissected from euthanized animals showed that most of the probes were located on the surface of the cells (bound to receptors on the surface) at 1 h, while at 3 h some of the probes were already detected in the intracellular pools, and internalization was almost complete by 48 h. In animals bearing MDA-MB231 and HT29 tumors, fluorescence signal in tumors dropped within the first 6 h after IntegriSense injection to a level that remained stable at least up to 24 h, and the specific fluorescence was still detectable up to 5–10 days. MDA-MB231 tumors had significantly higher levels of IntegriSense signal than HT29 from 4 to 24 h after injection (P < 0.05). Presence of 100-fold excess parent compound lowered the fluorescence in the MDA-MB231 tumor xenografts by 60% at 24 h after injection. A similar effect of the parent compound was observed in tumors derived from other cancer cell lines positive for α_v_β_3_ (data not shown).

In vivo imaging was performed on A673 tumor-bearing mice in the absence or presence of excess competing parent compound. Control mice received free dye. Fluorescence was readily detected in tumors. The total amount of IntegriSense fluorescence was significantly decreased in tumors of mice having received the parent compound (by 67% (P = 0.011)). Mice injected with free dye had significantly lower tumor signal than those injected with IntegriSense (P = 0.00038). After treatment of the tumor xenografts with Avastin for one week, IntegriSense signal in tumors decreased by 57% (P = 0.0008), reflecting a 58.3% decrease in tumor volume. Avastin is a monoclonal antibody against vascular endothelial growth factor.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Ruegg C., Alghisi G.C. (2010). Vascular integrins: therapeutic and imaging targets of tumor angiogenesis. Recent Results Cancer Res.
2 Desgrosellier J.S., Cheresh D.A. (2010). Integrins in cancer: biological implications and therapeutic opportunities. Nat Rev Cancer.
3 Caswell P.T., Vadrevu S., Norman J.C. (2009). Integrins: masters and slaves of endocytic transport. Nat Rev Mol Cell Biol.
4 Lim E.H., Danthi N., Bednarski M., Li K.C. (2005). A review: Integrin alphavbeta3-targeted molecular imaging and therapy in angiogenesis. Nanomedicine.
5 Schnell O., Krebs B., Wagner E., Romagna A., Beer A.J., Grau S.J., Thon N., Goetz C., Kretzschmar H.A., Tonn J.C., Goldbrunner R.H. (2008). Expression of integrin alphavbeta3 in gliomas correlates with tumor grade and is not restricted to tumor vasculature. Brain Pathol.
6 Beer A.J., Schwaiger M. (2008). Imaging of integrin alphavbeta3 expression. Cancer Metastasis Rev.
7 Blankenberg F.G., Mari C., Strauss H.W. (2002). Development of radiocontrast agents for vascular imaging: progress to date. Am J Cardiovasc Drugs.
8 Dijkgraaf I., Boerman O.C. (2009). Radionuclide imaging of tumor angiogenesis. Cancer Biother Radiopharm.
9 Kossodo, S., M. Pickarski, S.A. Lin, A. Gleason, R. Gaspar, C. Buono, G. Ho, A. Blusztajn, G. Cuneo, J. Zhang, J. Jensen, R. Hargreaves, P. Coleman, G. Hartman, M. Rajopadhye, L.T. Duong, C. Sur, W. Yared, J. Peterson, and B. Bednar, Dual In Vivo Quantification of Integrin-targeted and Protease-activated Agents in Cancer Using Fluorescence Molecular Tomography (FMT). Mol Imaging Biol, 2009
10 Stollman T.H., Ruers T.J., Oyen W.J., Boerman O.C. (2009). New targeted probes for radioimaging of angiogenesis. Methods.
11 Posey J.A., Khazaeli M.B., DelGrosso A., Saleh M.N., Lin C.Y., Huse W., LoBuglio A.F. (2001). A pilot trial of Vitaxin, a humanized anti-vitronectin receptor (anti alpha v beta 3) antibody in patients with metastatic cancer. Cancer Biother Radiopharm.
12 Gutheil J.C., Campbell T.N., Pierce P.R., Watkins J.D., Huse W.D., Bodkin D.J., Cheresh D.A. (2000). Targeted antiangiogenic therapy for cancer using Vitaxin: a humanized monoclonal antibody to the integrin alphavbeta3. Clin Cancer Res.
13 Liu S. (2006). Radiolabeled multimeric cyclic RGD peptides as integrin alphavbeta3 targeted radiotracers for tumor imaging. Mol Pharm.
14 Sillerud L.O., Larson R.S. (2005). Design and structure of peptide and peptidomimetic antagonists of protein-protein interaction. Curr Protein Pept Sci.
15 Yu M., Zhou H., Liu X., Huo Y., Zhu Y., Chen Y. (2010). Study on biodistribution and imaging of radioiodinated arginine-arginine-leucine peptide in nude mice bearing human prostate carcinoma. Ann Nucl Med.
16 Dijkgraaf I., Kruijtzer J.A., Liu S., Soede A.C., Oyen W.J., Corstens F.H., Liskamp R.M., Boerman O.C. (2007). Improved targeting of the alpha(v)beta (3) integrin by multimerisation of RGD peptides. Eur J Nucl Med Mol Imaging.
17 Dijkgraaf I., Beer A.J., Wester H.J. (2009). Application of RGD-containing peptides as imaging probes for alphavbeta3 expression. Front Biosci.
18 Weller G.E., Villanueva F.S., Tom E.M., Wagner W.R. (2005). Targeted ultrasound contrast agents: in vitro assessment of endothelial dysfunction and multi-targeting to ICAM-1 and sialyl Lewisx. Biotechnol Bioeng.
19 Coleman P.J., Brashear K.M., Askew B.C., Hutchinson J.H., McVean C.A. (2004). T. Duong le, B.P. Feuston, C. Fernandez-Metzler, M.A. Gentile, G.D. Hartman, D.B. Kimmel, C.T. Leu, L. Lipfert, K. Merkle, B. Pennypacker, T. Prueksaritanont, G.A. Rodan, G.A. Wesolowski, S.B. Rodan, and M.E. Duggan, Nonpeptide alphavbeta3 antagonists. Part 11: discovery and preclinical evaluation of potent alphavbeta3 antagonists for the prevention and treatment of osteoporosis. J Med Chem.
20 Wang J., Breslin M.J., Coleman P.J., Duggan M.E., Hunt C.A., Hutchinson J.H., Leu C.T., Rodan S.B., Rodan G.A. (2004). T. Duong le, and G.D. Hartman, Non-peptide alpha v beta 3 antagonists. Part 7: 3-Substituted tetrahydro-naphthyridine derivatives. Bioorg Med Chem Lett.
21 Luker G.D., Luker K.E. (2008). Optical imaging: current applications and future directions. J Nucl Med.
22 Graves E.E., Ripoll J., Weissleder R., Ntziachristos V. (2003). A submillimeter resolution fluorescence molecular imaging system for small animal imaging. Med Phys.